# ^99m^Tc-Hydrazinonicotinamide-anti-TAG-72 CC49 tetravalent single-chain Fv monoclonal antibody

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-anti-TAG-72 CC49 tetravalent single-chain Fv monoclonal antibody
Abbreviated name: | ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb
Synonym: | ^99m^Tc-CC49 [sc(Fv)_2_]_2_ MAb, ^99m^Tc-CC49 MAb
Agent Category: | Tetravalent single-chain Fv monoclonal antibody ([sc(Fv)_2_]_2_ MAb)
Target: | TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mtc-labeld+tetravalent+cc49single+chain+fv)+OR+(radiolabeled+cc49+scfv))]

^99m^Tc-Hydrazinonicotinamide-anti-TAG-72 CC49 tetravalent single-chain Fv monoclonal antibody (^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb), which is formed by the conjugation of ^99m^Tc with a bioengineered anti–tumor-associated glycoprotein 72 (TAG-72) antibody construct, has been developed for single-photon emission computed tomography (SPECT) imaging of cancers that express TAG-72 (1). ^99m^Tc is a gamma emitter with a half-life (t_½_) of 6.02 h.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (2-5). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (6). The murine monoclonal antibody B72.3 (MAb B72.3) against TAG-72 was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (7). With use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-2 monoclonal antibodies with higher affinity constants (K_a_) have been produced and characterized (1-3, 7).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (8). Radiolabeled B72.3 and CC49 have shown excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (9, 10). Because of their relatively large size, radiolabeled intact monoclonal antibodies tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (1, 11-13). One approach to minimize these problems is reducing intact antibodies to antibody fragments such as F(ab’)_2_ and Fab’. (14). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (1, 15, 16). These scFv constructs contain the variable regions of the light chain (V_L_) and heavy chain (V_H_) connected by a flexible linker. Colcher et al. (17) constructed the monomeric CC49 scFv MAb (~27 kDa), which selectively recognizes a unique sialyl-Tn epitope of TAG-72. The radioiodinated CC49 scFv appeared to clear rapidly from the blood with good tumor penetration (16, 18). To further improve the imaging kinetics, Pavlinkova et al. (18) constructed the high-affinity dimer CC49 sc(Fv)_2_ (~60 kDa). The radioiodinated CC49 sc(Fv)_2_ showed good stability and increased avidity in vivo compared with the radioiodinated CC49 scFv construct. Goel et al. (19) formed the tetravalent [sc(Fv)_2_]_2_ construct (~120 kDa) that exhibited four potentially active antigen-binding sites and showed improved in vitro binding properties.

MAbs can be labeled with ^99m^Tc, a gamma emitter with ideal SPECT imaging properties, by direct or indirect labeling. Direct labeling involves reduction of ^99m^Tc-pertechnetate and nonspecific binding of the reduced ^99m^Tc to donor atoms, namely thiol, amide, amino, and carboxylate (20). Indirect labeling uses a bifunctional chelating agent, which can be more binding site–specific on the MAb molecule. Goel et al. (1) used hydrazinonicotinamide (HYNIC) as a bifunctional coupling agent to label divalent CC49 sc(Fv)_2_ and tetravalent CC49 [sc(Fv)_2_]_2_ with ^99m^Tc. Both ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb and ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb showed good tumor targeting and in vivo biodistribution properties.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((99mtc-labeld+tetravalent+cc49single+chain+fv)+OR+(radiolabeled+cc49+scfv))+AND+synthesis)]

Goel et al. (1) reported the construction and radiolabeling of the ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb The CC49 scFv (V_L_-linker-V_H_) was derived from the murine MAb CC49 cloned in the yeast expression vector pPICZαA and constructed with the 205C linker with 25 amino acids. The bacterial scFv construct was used as the template DNA for the expression of the scFv in competent methylotrophic P. pastoris KM71 cells. The construction of the divalent sc(Fv)_2_ (V_L_-linker-V_H_-linker-V_L_-linker-V_H_-His_6_) was performed as described by Goel et al. (21) using the 205C linker in a P. pastoris expression system. On expression as a secreted protein by the P. pastoris, 20–30% of the divalent form was found to spontaneously associate through noncovalent interactions into the tetravalent [sc(Fv)_2_]_2_ or higher aggregates (>200 kDa) (19). The construct was purified from the secreted medium with immobilized metal affinity chromatography, and the [sc(Fv)_2_]_2_ was separated on a Superdex 200 column. The yield was reported to be 2.0–3.5 mg/liter. The preparation was shown to be >95% pure by sodium dodecylsulfate-polyacrylamide gel electrophoresis (SDS-PAGE). The SDS-PAGE study also confirmed that the two polypeptide chains of the tetramer were noncovalently linked. Size-exclusion high-performance liquid chromatography (HPLC) showed the molecular mass to be 120 kDa. Competitive solid-phase competition enzyme-linked immunosorbent assay (ELISA) with bovine submaxillary gland mucin (BSM) confirmed the immunoreactivity of the tetravalent construct with K_a_ = 1.0 × 10^8^ M−^1^. To radiolabel the agent, the hydrazino-modification of CC49 [sc(Fv)_2_] was achieved by reacting the construct with the N-hydroxysuccinimide ester of succinimidyl-6-hydrazinonicotinate hydrochloride (SHNH) at a molar ratio of 10:1 in sodium phosphate buffer (pH 7.8) in the dark at 4ºC overnight. It was estimated that there were ~2.8 SHNH groups per [sc(Fv)_2_]_2_. In the radiolabeling procedure, sodium ^99m^Tc-pertechnetate, tricine, and stannous chloride were first mixed, then SHNH-derivatized CC49 [sc(Fv)_2_]_2_ was added, and the reaction mixture was incubated at room temperature for 45 min. The final ^99m^Tc-HYNIC-CC49 [sc(FV)_2_]_2_ MAb was purified on a Sephadex G-25 column. The final radiochemical yield was not reported. The specific activity was 74–111 MBq/mg (2–3 mCi/mg) or 8.88–13.32 MBq/μmol (0.24–0.36 mCi/μmol) on the basis of the estimated 120-kDa molecular mass with a radiochemical purity ≥95% (HPLC analysis).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

The immunoreactivity of ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb by solid-phase ELISA with immobilized BSM was 85–95% with a nonspecific binding of 0.8–1.5% (1).

In vitro stability studies of ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb were conducted by incubating the radiolabeled MAb construct in 1% bovine serum albumin (BSA) or 1% mouse serum at 37ºC for 24 h (1). By HPLC analysis, <20% loss of ^99m^Tc label was detected in 1% BSA. In the 1% mouse serum, 65.2% of ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb remained intact, and 6.4% and 18.2% were associated with >130-kDa and <50-kDa proteins, respectively; ~10.2% of the ^99m^Tc radioactivity was associated with a 60-kDa protein. This suggested the possibility of dissociation of the tetramers to the dimmers.

Using the Scatchard plot and surface plasmon resonance technique to measure the real-time interactions, Goel et al. (19) reported the K_a_ of unlabeled CC49 [sc(Fv)_2_]_2_ to be 1.02 × 10^8^ M−^1^ in binding to the immobilized BSM. In comparison, the K_a_ for the intact CC49 MAb and CC49 sc(Fv)_2_ constructs were 1.14 × 10^8^ M−^1^ and 2.75 × 10^7^ M−^1^, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((99mtc-labeld+tetravalent+cc49single+chain+fv)+OR+(radiolabeled+cc49+scfv))+AND+rodentia)]

Biodistribution studies of ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb were performed in nude mice bearing LS-174T s.c. human colon carcinomas (~250–300 mm^3^) (1). Each mouse received 0.37 MBq (10 μCi) of ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb by i.v. administration. The blood elimination t_½_ was 307 min, and the whole-body clearance t_½_ was 265 ± 39 min (n = 3). The radioactivity levels (n = 3 × 2) in percentage injected dose per gram (% ID/g) of the tumors were 13.3 ± 1.4 (0.5 h), 14.5 ± 0.9 (1 h), 15.0 ± 1.2 (4 h), 19.1 ± 1.1 (6 h), 5.6 ± 0.2 (16 h), and 2.5 ± 0.0 (24 h). At 16 h, the tumor/blood ratio was 12.7:1 with tumor localization approximately three-fold higher than that of ^99m^Tc-sc(Fv_2_). At 0.5 h, the radioactivity levels (% ID/g) of major organs were 27.3 ± 1.5 (blood), 18.0 ± 1.3 (liver), 13.2 ± 0.8 (spleen), 17.2 ± 0.5 (kidneys), and 7.2 ± 1.1 (lungs). At 4 h, these levels changed to 7.5 ± 0.5 (blood), 20.1 ± 1.1 (liver), 10.9 ± 0.5 (spleen), 14.3 ± 1.9 (kidneys), and 2.7 ± 0.5 (lungs). By 24 h, these levels declined to 0.1 ± 0.0 (blood), 1.6 ± 0.0 (liver), 1.0 ± 0.0 (spleen), 1.1 ± 0.0 (kidneys), and 0.1 ± 0.0 (lungs). Macroautoradiography studies performed in mice at 6 h and 16 h after radioactivity administration confirmed a high degree of tumor localization and negligible retention in the blood and normal organs (1). The exceptions were the liver and pancreas. The tumor remained positive with decreased background radioactivity at 16 h after injection. In comparison, the radioactivity level of ^99m^Tc-HYNIC-CC49 [sc(Fv)_2_]_2_ MAb was about three-fold less than that of the divalent ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((99mtc-labeld+tetravalent+cc49single+chain+fv)+OR+(radiolabeled+cc49+scfv))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((((99mtc-labeld+tetravalent+cc49single+chain+fv)+OR+(radiolabeled+cc49+scfv))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((99mtc-labeld+tetravalent+cc49single+chain+fv)+OR+(radiolabeled+cc49+scFv))+AND+human)]

No publication is currently available.

## References

1 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
2 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
3 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
4 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
5 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
6 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
7 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
8 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
9 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
10 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
11 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
12 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
13 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
14 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
15 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
16 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
17 Colcher D., Goel A., Pavlinkova G., Beresford G., Booth B., Batra S.K. (1999). Effects of genetic engineering on the pharmacokinetics of antibodies. Q J Nucl Med.
18 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.
19 Goel A., Colcher D., Baranowska-Kortylewicz J., Augustine S., Booth B.J., Pavlinkova G., Batra S.K. (2000). Genetically engineered tetravalent single-chain Fv of the pancarcinoma monoclonal antibody CC49: improved biodistribution and potential for therapeutic application. Cancer Res.
20 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
21 Goel A., Beresford G.W., Colcher D., Pavlinkova G., Booth B.J., Baranowska-Kortylewicz J., Batra S.K. (2000). Divalent forms of CC49 single-chain antibody constructs in Pichia pastoris: expression, purification, and characterization. J Biochem (Tokyo).